# (S)-N-(1-Ethyl-2-pyrrolidinyl)methyl)-5-bromo-2-[^11^C]methoxy-3-methoxybenzamide

Chemical name: | (S)-N-(1-Ethyl-2-pyrrolidinyl)methyl)-5-bromo-2-[^11^C]methoxy-3-methoxybenzamide
Abbreviated name: | [^11^C]FLB 457
Synonym: | [^11^C]isoremoxipride
Agent Category: | Compound
Target: | Dopamine receptors (D_2_ and D_3_)
Target Category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20FLB%20457)]

Dopamine, a neurotransmitter, plays an important role in the mediation of movement, cognition, and emotion (1, 2). Dopamine receptors are involved in the pathophysiology of neuropsychiatric diseases, such as Parkinson’s disease (PD), Alzheimer's disease, Huntington’s disease, and schizophrenia (3). Five subtypes of dopamine receptors, D_1_ through D_5_, have been well characterized pharmacologically and biochemically (4). These five subtypes are classified into two subfamilies: D_1_-like (D_1_ and D_5_) and D_2_-like (D_2_, D_3_, and D_4_) dopamine receptors. D_1_-like and D_2_-like receptors exert synergistic as well as opposite effects at both the biochemical and overall system level. A great majority of striatal D_1_ and D_2_ receptors are localized postsynaptically on caudate-putamen neurons and to a lesser extent presynaptically on nigrostriatal axons. Extrastriatal dopamine receptors have also been suggested to play an important role in the pathophysiology of schizophrenia and other psychiatric disorders (5).

Substituted benzamides, such as sulpiride, raclopride, and iodobenzamide, are specific ligands with only moderate affinity for the D_2_ receptors, making studies of extrastriatal D_2_ receptors difficult (6-8). In binding studies, ^123^I-labeled epidepride, an analog of isoremoxipride, was found to have high potency and low nonspecific binding, and to be selective for striatal and extrastriatal D_2_ receptors (9). Epidepride has marginal binding to D_4_ receptors, with little affinity for other known neurotransmitter receptors. (S)-N-((1-Allyl-2-pyrrolidinyl)methyl)-5-(3-[^18^F]fluoropropyl)-2,3-dimethoxybenzamide ([^18^F]fallypride), an analog of epidepride, was found to be a selective, high-affinity antagonist (K_i_ = 0.03 nM) of D_2/3_ receptors (10), and in positron emission tomography (PET) in vivo studies (11-13). (S)-N-(1-Ethyl-2-pyrrolidinyl)methyl)-5-bromo-2,3-dimethoxybenzamide (FLB 457, or isoremoxipride) had very high affinity for D_2_ (K_i_ = 0.017 nM) and D_3_ (K_i_ = 0.022 nM) receptors but not other neurotransmitter receptors (14). [^11^C]FLB 457 has been used as a PET agent for the non-invasive study of extrastriatal D_2/3_ receptors in the human brain.

.

### Related Resource Links:

- Chapters in MICAD (Dopamine receptors (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=dopamine%20(receptors%20OR%20receptor)+%20AND+Table+AND+micad%5Bbook%5D))
- Gene information in NCBI (D_2_ receptor, (http://www.ncbi.nlm.nih.gov/gene/1813) D_3_ receptor (http://www.ncbi.nlm.nih.gov/gene/1814))
- Articles in Online Mendelian Inheritance in Man (OMIM) (D_2_ receptor (http://www.ncbi.nlm.nih.gov/omim/126450), D_3_ receptor (http://www.ncbi.nlm.nih.gov/omim/126451))
- Clinical trials (Dopamine receptors (http://www.clinicaltrials.gov/ct2/results?term=dopamine+receptor))
- Drug information in Food and Drug Administration (Dopamine receptors (http://google2.fda.gov/search?q=dopamine+receptor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=6&y=12))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20FLB%20457%20and%20synthesis)]

Halldin et al. (14) reported that they synthesized [^11^C]FLB 457 by direct O-methylation of 2-hydroxy-FLB 457 with [^11^C]methyl iodide and NaOH in dimethyl sulfoxide, with a radiochemical yield of 25-35% (end of bombardment) and an average specific activity of 48 GBq/μmol (1,300 Ci/mmol at end of synthesis) after high-performance liquid chromatography (HPLC) purification. Radiochemical purities were >99% with a total synthesis time of 30 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20FLB%20457%20and%20in%20vitro)]

In vitro binding assays showed that FLB 457 had high affinities for D_2_ (K_i_ = 0.022 ± 0.001 nM) and D_3_ (K_i_ = 0.017 ± 0.001 nM) receptors but not D_1_, α_1_, α_2_, 5-HT_1A_, and 5-HT_2_ receptors (14). These results indicate that FLB 457 binds equally well to D_2_ and D_3_ receptors.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20FLB%20457%20and%20rodentia)]

Biodistribution studies by Ahmad et al. (15) in rats showed rapid accumulation of radioactivity in all brain regions within minutes after injection of [^11^C]FLB 457. Thereafter, radioactivity accumulated further only in the striata. On the other hand, all other regions showed various washout rates. Kinetic analysis with a two-tissue model using plasma input function (5 samples/rat) was used to derive the binding potential (BP) of each region. The striatum had the highest BP (83), followed by the inferior colliculi (11.0), olfactory tubercles (5.9), superior colliculi (5.1), hypothalamus (3.3), pons with medulla (2.7), thalamus (2.5), frontal cortex (2.3), prefrontal cortex (2.1), hippocampus (1.8), occipital cortex (1.1), and cerebellum (0.8). Thus, the hypothalamus, prefrontal cortex, and cerebellum represent extrastriatal tissues with moderate, low, and minimal D_2/3_ receptor density. Apparent K_d_ values were in the range of 2-3 nmol/kg in the extrastriatal regions. The extrastriatal basal occupancy by dopamine was minimal (<10%). [^11^C]FLB 457 thus displays uptake and washout kinetics characteristic of reversible radiotracers.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20FLB%20457%20and%20%28Pig%20or%20dog%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20FLB%20457%20and%20%28primate%20not%20human%29)]

Halldin et al. (14) performed PET studies with [^11^C]FLB 457 in three cynomolgus monkeys and found rapid accumulation in the brain (3.5% of injected radioactivity) at 4 min after injection. The highest uptake was in the striatum, with striatum/cerebellum ratios of 15 at 60 min and 25 at 93 min after injection of 37 MBq (1 mCi) of [^11^C]FLB 457. The thalamus/cerebellum and neocortex/cerebellum ratios were 4.0 and 2.5. The accumulation of [^11^C]FLB 457 in the striatum, thalamus, and neocortex was almost completely displaced after injection of raclopride (1 mg/kg) or haloperidol (2 mg/kg) at 15-20 min after the tracer injection. The fraction of unchanged [^11^C]FLB 457 in plasma, as determined by HPLC, was 80 and 34% at 5 and 86 min after injection, respectively. All radiolabeled metabolites were more hydrophilic than the parent compound and not expected to cross the blood-brain barrier.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20FLB%20457%20and%20human)]

[^11^C]FLB 457 PET studies of D_2/3_ receptor distribution in human brain have been reported, showing major localization of radioactivity in the striata and significant minor accumulation in the extrastriatal regions. Quantitative analysis of [^11^C]FLB 457 binding was usually performed to derive BPs (with cerebellum as reference) to measure receptor concentrations. Olsson et al. (16) reported on [^11^C]FLB 457 PET studies in eight normal subjects (23-38 years of age), using the standard three-compartment model with arterial input function. PET brain scans showed high accumulation of radioactivity in the putamen (BP = 19.04 ± 10.8), followed by the thalamus (BP = 2.82 ± 0.46), temporal cortex (BP = 1.29 ± 0.23), anterior cinguli (BP = 0.76 ± 0.17), and frontal cortex (BP = 0.65 ± 0.13), with good reproducibility. However, the short time of a PET measurement using [^11^C]FLB 457 (63 min) seemed insufficient for reliable determination of the high BP in the striatum.

Farde et al. (17) found that pretreatment with haloperidol and fluphenazine blocked [^11^C]raclopride binding in the striatum and [^11^C]FLB 457 binding in the thalamus and neocortex in two healthy subjects and two patients with schizophrenia. Subsequent studies by Vilkman et al. (18) and Sudo et al. (19) showed good test-retest reproducibility for [^11^C]FLB 457 binding in extrastriatal regions in normal subjects. Two other groups (20, 21) found that there was an age-dependent decrease (>10% per decade) of [^11^C]FLB 457 binding in most extrastriatal regions (decreases of 5-5% per decade in the thalamus and 7% in the amygdale) in healthy volunteers.

Kaasinen et al. (22) reported on a [^11^C]FLB 457 PET study of 14 drug-naive patients with idiopathic early PD with predominantly left-sided symptoms, 14 levodopa-medicated patients with advanced PD, and 20 normal age-matched controls. In advanced PD, the BP of [^11^C]FLB 457 was decreased by 40% (P < 0.01) in the dorsolateral prefrontal cortex, by 20% (P < 0.01) in the anterior cingulate cortex, and by 17% (P < 0.05) in the medial thalamus compared with healthy controls. In early PD, the extrastriatal [^11^C]FLB 457 BPs were not significantly different compared with the control group. However, the BP in the anterior cingulate cortex (29%; P < 0. 05) was higher in early PD compared with advanced PD. This indicates that the D_2/3_ receptor subtypes outside the striatum are affected in advanced PD but not in the early stages of the disease and that this receptor decline is present in the anterior cingulate cortex, the dorsolateral prefrontal cortex, and the thalamus.

Talvik et al. (23) studied extrastriatal binding of [^11^C]FLB 457 binding for D_2/3_ receptor sites in nine drug-naive patients (36 ± 12 years of age) with schizophrenia and in eight healthy control subjects (31 ± 12 years of age). The patients exhibited significantly lower BP values (3.13 ± 0.33) than the healthy controls (4.06 ± 1.05) in the right medial thalamus. There was also a significant decrease in BPs with age in the frontal and temporal cortex for both groups.

Aalto et al. (24) compared regional brain BPs of [^11^C]FLB 457 in eight normal volunteers with ketamine infusion and eight normal volunteers. There was a significant decrease in [^11^C]FLB 457 BP in the posterior cingulated/retrosplenial cortices of ketamine-infused subjects compared with controls, suggesting an increase in dopamine release. No significant differences were observed in other cortical regions. Ketamine-induced psychotic symptoms were associated with changes in the [^11^C]FLB 457 BP in the dorsolateral prefrontal and anterior cingulated cortices. This is similar to what was found by Breier et al. (25) using ketamine and [^11^C]raclopride.

[^11^C]FLB 457 PET is useful for objective monitoring of D_2/3_ receptor binding and drug occupancy in patients with dopaminergic disorders. Internal dosimetry data for [^11^C]FLB 457 in humans are not available in the literature.

## References

1 Carbon M., Ghilardi M.F., Feigin A., Fukuda M., Silvestri G., Mentis M.J., Ghez C., Moeller J.R., Eidelberg D. (2003). Learning networks in health and Parkinson's disease: reproducibility and treatment effects. Hum Brain Mapp.
2 Chesselet M.F., Delfs J.M. (1996). Basal ganglia and movement disorders: an update. Trends Neurosci.
3 Seeman P., Bzowej N.H., Guan H.C., Bergeron C., Reynolds G.P., Bird E.D., Riederer P., Jellinger K., Tourtellotte W.W. (1987). Human brain D1 and D2 dopamine receptors in schizophrenia, Alzheimer's, Parkinson's, and Huntington's diseases. Neuropsychopharmacology.
4 Stoof J.C., Kebabian J.W. (1984). Two dopamine receptors: biochemistry, physiology and pharmacology. Life Sci.
5 Lidow M.S., Williams G.V., Goldman-Rakic P.S. (1998). The cerebral cortex: a case for a common site of action of antipsychotics. Trends Pharmacol Sci.
6 Gehlert D.R., Wamsley J.K. (1984). Autoradiographic localization of [3H]sulpiride binding sites in the rat brain. Eur J Pharmacol.
7 Lidow M.S., Goldman-Rakic P.S., Rakic P., Innis R.B. (1989). Dopamine D2 receptors in the cerebral cortex: distribution and pharmacological characterization with [3H]raclopride. Proc Natl Acad Sci U S A.
8 Brucke T., Tsai Y.F., McLellan C., Singhanyom W., Kung H.F., Cohen R.M., Chiueh C.C. (1988). In vitro binding properties and autoradiographic imaging of 3-iodobenzamide ([125I]-IBZM): a potential imaging ligand for D-2 dopamine receptors in SPECT. Life Sci.
9 Kessler R.M., Ansari M.S., Schmidt D.E., de Paulis T., Clanton J.A., Innis R., al-Tikriti M., Manning R.G., Gillespie D. (1991). High affinity dopamine D2 receptor radioligands. 2. [125I]epidepride, a potent and specific radioligand for the characterization of striatal and extrastriatal dopamine D2 receptors. Life Sci.
10 Mukherjee J., Yang Z.Y., Das M.K., Brown T. (1995). Fluorinated benzamide neuroleptics--III. Development of (S)-N-[(1-allyl-2-pyrrolidinyl)methyl]-5-(3-[18F]fluoropropyl)-2, 3-dimethoxybenzamide as an improved dopamine D-2 receptor tracer. Nucl Med Biol.
11 Grunder G., Landvogt C., Vernaleken I., Buchholz H.G., Ondracek J., Siessmeier T., Hartter S., Schreckenberger M., Stoeter P., Hiemke C., Rosch F., Wong D.F., Bartenstein P. (2006). The striatal and extrastriatal D2/D3 receptor-binding profile of clozapine in patients with schizophrenia. Neuropsychopharmacology.
12 Mukherjee J., Christian B.T., Narayanan T.K., Shi B., Collins D. (2005). Measurement of d-amphetamine-induced effects on the binding of dopamine D-2/D-3 receptor radioligand, 18F-fallypride in extrastriatal brain regions in non-human primates using PET. Brain Res.
13 Riccardi P., Li R., Ansari M.S., Zald D., Park S., Dawant B., Anderson S., Doop M., Woodward N., Schoenberg E., Schmidt D., Baldwin R., Kessler R. (2006). Amphetamine-induced displacement of [18F] fallypride in striatum and extrastriatal regions in humans. Neuropsychopharmacology.
14 Halldin C., Farde L., Hogberg T., Mohell N., Hall H., Suhara T., Karlsson P., Nakashima Y., Swahn C.G. (1995). Carbon-11-FLB 457: a radioligand for extrastriatal D2 dopamine receptors. J Nucl Med.
15 Ahmad R., Hirani E., Grasby P.M., Hume S.P. (2006). Effect of reduction in endogenous dopamine on extrastriatal binding of [11C]FLB 457 in rat brain--an ex vivo study. Synapse.
16 Olsson H., Halldin C., Swahn C.G., Farde L. (1999). Quantification of [11C]FLB 457 binding to extrastriatal dopamine receptors in the human brain. J Cereb Blood Flow Metab.
17 Farde L., Suhara T., Nyberg S., Karlsson P., Nakashima Y., Hietala J., Halldin C. (1997). A PET-study of [11C]FLB 457 binding to extrastriatal D2-dopamine receptors in healthy subjects and antipsychotic drug-treated patients. Psychopharmacology (Berl).
18 Vilkman H., Kajander J., Nagren K., Oikonen V., Syvalahti E., Hietala J. (2000). Measurement of extrastriatal D2-like receptor binding with [11C]FLB 457--a test-retest analysis. Eur J Nucl Med.
19 Sudo Y., Suhara T., Inoue M., Ito H., Suzuki K., Saijo T., Halldin C., Farde L. (2001). Reproducibility of [11 C]FLB 457 binding in extrastriatal regions. Nucl Med Commun.
20 Inoue M., Suhara T., Sudo Y., Okubo Y., Yasuno F., Kishimoto T., Yoshikawa K., Tanada S. (2001). Age-related reduction of extrastriatal dopamine D2 receptor measured by PET. Life Sci.
21 Kaasinen V., Vilkman H., Hietala J., Nagren K., Helenius H., Olsson H., Farde L., Rinne J. (2000). Age-related dopamine D2/D3 receptor loss in extrastriatal regions of the human brain. Neurobiol Aging.
22 Kaasinen V., Nagren K., Hietala J., Oikonen V., Vilkman H., Farde L., Halldin C., Rinne J.O. (2000). Extrastriatal dopamine D2 and D3 receptors in early and advanced Parkinson's disease. Neurology.
23 Talvik M., Nordstrom A.L., Olsson H., Halldin C., Farde L. (2003). Decreased thalamic D2/D3 receptor binding in drug-naive patients with schizophrenia: a PET study with [11C]FLB 457. Int J Neuropsychopharmacol.
24 Aalto S., Ihalainen J., Hirvonen J., Kajander J., Scheinin H., Tanila H., Nagren K., Vilkman H., Gustafsson L.L., Syvalahti E., Hietala J. (2005). Cortical glutamate-dopamine interaction and ketamine-induced psychotic symptoms in man. Psychopharmacology (Berl).
25 Breier A., Malhotra A.K., Pinals D.A., Weisenfeld N.I., Pickar D. (1997). Association of ketamine-induced psychosis with focal activation of the prefrontal cortex in healthy volunteers. Am J Psychiatry.